# Bovine serum albumin–stabilized gold nanoclusters conjugated with L-methionine and indocyanine green derivative 02

Chemical name: | Bovine serum albumin–stabilized gold nanoclusters conjugated with L-methionine and indocyanine green derivative 02
Abbreviated name: | Au-Met-MPA
Synonym: | Au-BSA-Met-MPA, Au-BSA-Met-ICG-Der-02, Au-Met-ICG-Der-02
Agent category: | Compound
Target: | L-type amino acid transporter 1/2 (LAT1/2)
Target category: | Transporter
Method of detection: | Optical, near-infrared fluorescence (NIR) imaging
Source of signal: | ICG-Der-02 (MPA)
Activation: | No
Studies: | - In vitro; - Rodents | Structure is not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Au-Met-MPA)]

Most amino acids are taken up by tumor cells through an energy-independent L-type amino acid transporter system, a Na-dependent transporter system A, or a Na^+^-dependent system B^0^ (1). They are retained in tumor cells due to their metabolic activities, including incorporation into proteins, which are higher than most normal cells (2). Malignant transformation increases the use of amino acids for energy, protein synthesis, and cell division. Tumor cells have been found to have overexpressed transporter systems (3). S-[^11^C]Methyl-L-methionine ([^11^C]MET) has been widely used in the detection of brain, head and neck, lung, and breast cancers as well as lymphomas (4) [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20methionine%20and%20human%20and%20neoplasm)]. [^11^C]MET can cross the blood–brain barrier, and while it is incorporated mainly into proteins, [^11^C]MET is also incorporated into lipid, RNA, and DNA. Positron emission tomography (PET) imaging with [^11^C]MET is more sensitive to radiotherapy compared to [^18^F]FDG and is useful for monitoring treatment of cancer.

Among the various optical imaging agents, only indocyanine green (ICG (http://dailymed.nlm.nih.gov/dailymed/drugInfo.cfm?id=15096)), with NIR fluorescence absorption at 780 nm and emission at 820 nm, is approved by the United States Food and Drug Administration for clinical applications in angiography, blood flow evaluation, and liver function assessment (5-8). It is also under evaluation in several clinical trials (http://clinicaltrials.gov/ct2/results?term=indocyanine+green) for other applications, such as optical imaging and mapping of both the lymphatic vessels and lymph nodes in cancer patients for surgical dissection of tumor cells and endoscopic imaging of the pancreas and colon. Gold (Au) nanoclusters (NCs) are comprised of a few tens of Au atoms that possess the ability to emit strong fluorescence, of which the wavelength is tunable in the range of the visible to near-infrared spectral region (9). Chen et al. (10) prepared bovine serum albumin–stabilized Au NCs (Au-BSA) for conjugation with biomolecules for specific targeting and with near-infrared dye for optical imaging. Met was conjugated to the carboxyl groups of BSA. The ICG derivative 02 (ICG-Der-02, also known as MPA) contains one carboxyl functional group for covalent conjugation to the amino group of BSA on the surface of Au-BSA NCs. MPA is a hydrophilic dye. Chen et al. (10) evaluated Au-BSA-Met-MPA (Au-Met-MPA) for in vivo NIR optical imaging in tumor-bearing mice.

### Related Resource Links:

- Chapters in MICAD (amino acid transporters (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=amino%20acid%20(transporter%20OR%20transporters)+AND+micad%5Bbook%5D), methionine (http://www.ncbi.nlm.nih.gov/books?term=methionine%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D), ICG (http://www.ncbi.nlm.nih.gov/books?term=ICG%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (L-type amino acid transporter 1 (http://www.ncbi.nlm.nih.gov/gene/8140), L-type amino acid transporter 2 (http://www.ncbi.nlm.nih.gov/gene/23428), A-type amino acid transporter (http://www.ncbi.nlm.nih.gov/gene/54407))
- Articles in Online Mendelian Inheritance in Man (OMIM) (amino acid transporters (http://www.ncbi.nlm.nih.gov/omim?Db=omim&Cmd=DetailsSearch&Term=amino%5BAll+Fields%5D+AND+acid%5BAll+Fields%5D+AND+transporter%5BAll+Fields%5D))
- Clinical trials (amino acid transporters (http://www.clinicaltrials.gov/ct2/results?term=amino+acid+transporters), L-[^11^C]methionine (http://www.clinicaltrials.gov/ct2/results?term=11C+MET), ICG (http://www.clinicaltrials.gov/ct2/results?term=ICG))
- Drug information in FDA (amino acid transporters (http://google2.fda.gov/search?q=amino+acid+transporters&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=13&y=15), ICG (http://google2.fda.gov/search?q=Indocyanine+Green&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=4&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Au-Met-MPA%20and%20synthesis)]

Au-BSA NCs were prepared by addition of HAuCl_4_ solution (10 mM) to BSA solution (50 mg/ml) under vigorous stirring for 30 min at 37°C (10). The mixture was stirred for an additional 12 h at 37°C. Au-BSA NCs were incubated with 1-ethyl-3-[3-dimethylaminopropyl]carbodiimide hydrochloride for 10 min at room temperature. N-Hydroxysuccinimide (NHS) was then incubated with the mixture for 2 h, after which Met was added and incubated for 12 h. The product, Au-BSA-Met, was isolated with column chromatography. MPA (1.0 mg) was activated with N,N'-dicyclohexylcarbodiimide (DDC) and NHS (molar ratio of MPA:DCC:NHS was 1:1.5:1.5) for 3 h at room temperature. Finally, the above activated MPA was evenly mixed with purified Au-BSA-Met and then incubated for 12 h at room temperature with stirring to produce Au-Met-MPA. The mean hydrodynamic diameter of Au-BSA (measured with laser particle size analysis) was 3.9 nm (polydispersity = 0.303), whereas Au-Met-MPA exhibited a relatively larger diameter of 5.6 nm (polydispersity = 0.118), indicating the successful addition of Met and MPA molecules. The absorption spectra of Met, Au-BSA, MPA, Au-BSA-Met, and Au-Met-MPA exhibited absorbance peaks at 215, 232, and 780 nm, which corresponded to Met, Au, and MPA, respectively. The number of Au, BSA, Met, and MPA moieties per Au-Met-MPA was not reported. Au-Met-MPA displayed spectral properties similar to those of MPA, with maximum absorption at 750 nm and maximum emission at 830 nm.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Au-Met-MPA%20and%20in%20vitro)]

The cytotoxic effects of Au-BSA, Au-BSA-Met, Au-BSA-MPA, and Au-Met-MPA (0.01–1,000 µM) were assessed in human cell lines L02 (normal human liver cell), Bel 7402 (liver cancer), A549 (lung cancer), and MCF-7 (breast cancer) for 24 h at 37°C (10). Approximately 90% viability was observed with 0.01–1 µM, with 80% at 1 mM. Fluorescence microscopy analysis showed little binding of Au-BSA and Au-Met-MPA to L02 cells (low LAT1/2 expression), whereas strong fluorescence signal was observed in the MCF-7 cells (high LAT1/2 expression) with Au-Met-MPA but not with Au-BSA-MPA. No blocking studies were performed with excess Met.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Au-Met-MPA%20and%20rodentia)]

Chen et al. (10) performed in vivo whole-body NIR fluorescence imaging studies in nude mice (the number of mice used was not reported) bearing MDA-MB-231 human breast cancer (high LAT1/2 expression) and A549 human lung cancer xenografts (low LAT1/2 expression) at 0.5–96 h after intravenous injection of Au-Met-MPA (10 mg/kg body weight). Images showed that NIR fluorescence spread all over the body at 0.5 h and then concentrated in the liver and kidneys. Most NIR fluorescence of the normal tissues was cleared from the body by 10 h. MDA-MB-231 tumors were clearly visualized at 2 h, and the NIR fluorescence peaked at 10 h. The tumor NIR fluorescence was still detectable at 96 h. On the other hand, A549 tumor exhibited weak NIR fluorescence at 2–4 h, and fluorescence was almost indistinguishable from the background by 7 h. The tumor/background ratio was 1.47 ± 0.16 at 0.5 h for MDA-MB-231 tumors, reaching a peak at 10 h (6.86 ± 0.12) and slowly declining to 2.83 ± 0.18 at 96 h. Au-Met-MPA exhibited little histological change in the excised organs from normal mice at 7 d after injection of Au-Met-MPA.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Au-Met-MPA%20and%20%28pig%20or%20dog%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Au-Met-MPA%20AND%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Au-Met-MPA%20and%20human)]

No publication is currently available.

## References

1 Langen K.J., Jarosch M., Muhlensiepen H., Hamacher K., Broer S., Jansen P., Zilles K., Coenen H.H. (2003). Comparison of fluorotyrosines and methionine uptake in F98 rat gliomas. Nucl Med Biol.
2 Jager P.L., Vaalburg W., Pruim J., de Vries E.G., Langen K.J., Piers D.A. (2001). Radiolabeled amino acids: basic aspects and clinical applications in oncology. J Nucl Med.
3 Saier M.H., Daniels G.A., Boerner P., Lin J. (1988). Neutral amino acid transport systems in animal cells: potential targets of oncogene action and regulators of cellular growth. J Membr Biol.
4 Laverman P., Boerman O.C., Corstens F.H., Oyen W.J. (2002). Fluorinated amino acids for tumour imaging with positron emission tomography. Eur J Nucl Med Mol Imaging.
5 Yannuzzi, L.A., Indocyanine green angiography: a perspective on use in the clinical setting. Am J Ophthalmol, 2011151(5): p. 745-751 e1.
6 Yamamoto M., Sasaguri S., Sato T. (2011). Assessing intraoperative blood flow in cardiovascular surgery. Surg Today.
7 Schaafsma B.E., Mieog J.S., Hutteman M., van der Vorst J.R., Kuppen P.J., Lowik C.W., Frangioni J.V., van de Velde C.J., Vahrmeijer A.L. (2011). The clinical use of indocyanine green as a near-infrared fluorescent contrast agent for image-guided oncologic surgery. J Surg Oncol.
8 Manizate F., Hiotis S.P., Labow D., Roayaie S., Schwartz M. (2010). Liver functional reserve estimation: state of the art and relevance for local treatments: the Western perspective. J Hepatobiliary Pancreat Sci.
9 Huang C.C., Chen C.T., Shiang Y.C., Lin Z.H., Chang H.T. (2009). Synthesis of fluorescent carbohydrate-protected Au nanodots for detection of Concanavalin A and Escherichia coli. Anal Chem.
10 Chen H., Li B., Ren X., Li S., Ma Y., Cui S., Gu Y. (2012). Multifunctional near-infrared-emitting nano-conjugates based on gold clusters for tumor imaging and therapy. Biomaterials.